# (R)-(+)-8-Chloro-2,3,4,5-tetrahydro-3-[^11^C]methyl-5-phenyl-1H-3-benzazepin-7-ol ([^11^C]SCH 23390)

Chemical name: | (R)-(+)-8-Chloro-2,3,4,5-tetrahydro-3-[^11^C]methyl-5-phenyl-1H-3-benzazepin-7-ol
Abbreviated name: | [^11^C]SCH 23390, [^11^C]SCH
Synonym:
Agent Category: | Compound
Target: | Dopamine D_1_ receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_-_5_, were well-characterized pharmacologically and biochemically (4). These five subtypes were classified into two subfamilies of D_1_-like (D_1_, D_5_) and D_2_-like (D_2_, D_3_, D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at the biochemical and overall system levels. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on the caudate-putamen neurons and to a lesser extent presynaptically on nigrostiatal axons.

(R)-(+)-8-Chloro-2,3,4,5-tetrahydro-3-[^11^C]methyl-5-phenyl-1H-3-benzazepin-7-ol ([^11^C]SCH 23390) was found to be a selective, high-affinity antagonist of D_1_ receptors. SCH 23390 was found to have marginal effect on D_2_, α_1_-adrenergic, muscarinic and histaminergic receptors and only a slight effect on 5-HT_2A_ receptors (5). [^11^C]SCH 23390 positron emission tomography (PET) has been used to study D_1_ receptor occupancy and density in neuropsychiatric disorders and aging in humans.

.

### Related Resource Links:

- Chapters in MICAD (Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_1_ receptor (http://www.ncbi.nlm.nih.gov/gene/1812))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_1_ receptor (http://www.ncbi.nlm.nih.gov/omim/126449))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))
- Drug information in Food and Drug Administration (Dopamine receptors (http://google2.fda.gov/search?q=dopamine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20synthesis)]

[^11^C]SCH 23390, was synthesized by alkylation of the desmethyl compound SCH 24518 ((R)-(+)-8-chloro-2,3,4,5-tetrahydro-5-phenyl-1H-3-benzazepin-7-ol) with [^11^C]methyl iodide (6). Reaction in acetone with subsequent normal-phase LC separation resulted in 80% radiochemical yield, based on [^11^C]methyl iodide, with a total synthesis time of 35-40 min and a radiochemical purity greater than 99%. The averaged specific activity was 11.1 GBq/mmol (300 Ci/mmol) at end of synthesis (EOS).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20in%20vitro)]

SCH 23390 was reported to have selective binding affinity to D_1_ (striatum) and 5-HT_2A_ (frontal cortex) receptor sites in homogenates of rat brain membranes (7). The K_i_ values for D_1_ ([^3^H]piflutixol), D_2_ ([^3^H]spiroperidol) in the striatal membranes and 5-HT_2A_ ([^3^H]spiroperidol) in the cortical membranes were 1.3 nM, 880 nM and 30 nM, respectively. It has a K_i_ value of 690 nM for the α_1_-adrenergic receptor in rat forebrain membrane. The affinity for the 5-HT_2A_ receptor is about 10-fold lower than that for the D_1_ receptor, suggesting that specific [^11^C]SCH 23390 binding visualized by PET represents mainly binding to D_1_ receptors. The K_d_ value of [^3^H]SCH 23390 was 0.53 nM for D_1_(8). The B_max_ value of [^3^H]SCH 23390 for D_1_ was 69 pmol/g tissue.

Using human putamen homogenates, the K_d_ values of [^3^H]SCH 23390 and [^3^H]raclopride, a D_2_ antagonist, were 1.6 ± 0.22 nM (1.1 ± 0.38 nM with 40 nM ketanserin, a 5-HT_2A_ antagonist) and 2.0 ± 0.2 nM, respectively (9). The D_1_ receptor binding density (B_max_) was 12.7 ± 3.8 and 9.9 ± 2.1 pmol/g tissue for [^3^H]SCH 23390 without and with 40 nM ketanserin, respectively. The B_max_ of [^3^H]raclopride for D_2/3_ receptor was 13.3 ± 0.9 pmol/g tissue. Using frontal cortex membranes, the B_max_ for D_1_ was 6.7 ± 3.9 and 3.3 ± 0.82 pmol/g tissue without and with 40 nM ketanserin, respectively. Ketanserin had little effect on the K_d_ (2.1 - 2.4 nM). There was little specific binding of raclopride in the cortex membranes. Therefore, part of the [^3^H]SCH 23390 bindings to the putamen and frontal cortex was due to 5-HT_2a_ receptor sites.

Hyttel (10) reported that the B_max_ and K_d_ of dopamine D_1_ and D_2_ receptors in striatum was estimated in rats of different ages (from 3.5 to 25 months) using [^3^H]SCH 23390 and [^3^H]spiperone as ligands. The density of D_1_ and D_2_ receptors decreased with age from 3.5 months’ values of 990 ± 50 and 350 ± 11 pmol/g tissue to 25 months’ values of 690 ± 35 (30% decrease) and 240 ± 7 pmol/g tissue (31% decrease), respectively. However, the K_d_ vaukes remained constant. The decreases in density of D_1_ and D_2_ receptors were parallel. Thus, the ratio between the density of D_1_ and D_2_ receptors remained constant throughout life

Hess et al (11) demonstrated that D_1_ receptor density ([^3^H]SCH 233900) was reduced by 43% in postmortem caudate brains from 8 schizophrenic patients as compared with 8 normal subjects from 281.5 ± 20.5 to 161.4 ± 22.1 fmol/mg protein. In contrast, schizophrenic patients exhibited a 56% increase in D_2_ receptor density from 119.8 ± 13.7 to 186.7 ± 33.0 fmol/mg protein as measured by [^3^H]spiperone in the presence of 40 nM ketanserin. These resulted in a highly significant difference in the ratio of D_2_/D_1_ receptor density between schizophrenic patients (1.29 ± 0.29) and controls (0.42 ± 0.03).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20rodentia)]

Biodistribution studies in mice showed a high accumulation of radioactivity in the intestines (1.38% injected dose (ID)/g), followed by the liver (1.06% ID/g), kidney (0.40% ID/g), lung (0.22% ID/g), and brain (0.17% ID/g) at 60 min after injection of [^11^C]SCH 23390. There was a rapid accumulation of the tracer in the striata within the first ten min (4.88% ID/g), followed by a slow decrease of radioactivity to 2.25% ID/g at 60 min. In contrast, radioactivity in the cerebellum decreased continuously from 1 min (3.10% ID/g) to 60 min (0.10% ID/g). The striatum-to-cerebellum ratios were 1.3, 3.1, 6.1, and 23.4 at 1, 10, 30, and 60 min, respectively.

Suzuki et al (12) reported that the binding potential (B_max_/K_d_) of [^11^C]SCH 23390 as measured by PET in the rat striata decreased as a function of age by a maximum of 26%, whereas the binding potential of [^11^C]raclopride decreased by 36%. These PET results confirmed the decreases in density of D_1_ and D_2/3_ receptors were parallel in aging rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20%28pig%20or%20rabbit%20or%20dog%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20%28primate%20not%20human%29)]

The distributions of dopamine D_1_ and D_2_ receptors in 6 monkeys were compared directly using PET (13). The binding potentials of [^11^C]SCH 23390 for dopamine D_1_ receptors and [^11^C]raclopride for dopamine D_2_ receptors were calculated in monkey striatum volumes of interest using cerebellum as a non-binding reference region. The D_1_ binding potential for [^11^C]SCH 23390 was 1.30 ± 0.04 in monkey striata, whereas the D_2_ binding potential for [^11^C]raclopride was 1.96 ± 0.44. There were distinct gradients in the distributions of the two binding sites in monkey brain: D_1_ binding predominated in the antero-ventral striatum, whereas D_2_ binding was relatively greater in the dorsal-posterior striatum.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20human)]

[^11^C]SCH 23390 PET studies of D_1_ receptor distribution in human brain were reported, showing a major localization of radioactivity in the striatum. Striatum-to-cerebellum ratio and kinetic constants are commonly used as analytical parameters in [^11^C]SCH 23390 PET studies with good reproducibility (14-16). Farde et al. (17) reported on [^11^C]SCH 23390 PET studies in 2 patients with schizophrenia and in 3 normal subjects. PET brain scans of normal subjects showed that a high accumulation of radioactivity was in the putamen, followed by the neocortex and cerebellum at 5 - 60 min after injection of 100 MBq (2.7 mCi) [^11^C]SCH 23390. The putamen-to-cerebellum ratio was 3 at 25 min. There was a marked accumulation of radioactivity in the neocortex for [^11^C]SCH 23390 but not for [^11^C]raclopride (D_2/3_ receptors), suggesting the presence of 5-HT_2A_ binding sites. Only about 1.2% of injected [^11^C]SCH 23390 remained in the brain at 4.5 min. Only 15% of radioactivity remained intact in blood at 42 min. PET scans of schizophrenic patients was similar to those obtained in the normal controls. [^11^C]SCH 23390 PET was able to assess striatal dopamine receptor occupancies in patients treated with various antipsychotic drugs (18).

The effects of age on the binding of [^11^C]SCH 23390 for D_1_ receptor sites were studied in 17 healthy male subjects in age from 20 to 72 years old (19). The binding potential of the D_1_ receptors in the striatum and frontal cortex decreased with age by 35% and 39%, respectively. In another study with 8 men and 10 women (22-74 years old) (20), there was an age dependent decrease of D_1_ receptor binding potential in the caudate, putamen, and occipital cortex by 6.9%/decade, 7.4%/decade, and 8.6%/decade, respectively. There was no difference in D_1_ binding potentials between men and women.

In Huntington’s disease, there was a significant reduction in both the D_1_ ([^11^C]SCH 23390) and D_2_ ([^11^C]raclopride) binding potentials in the striatum (21-23). A great majority (90%) of patients was not on any medication affecting the dopamine and serotonin system. Medications were withdrawn for 1 to 14 days prior to PET. In Parkinson’s disease, there was no significant difference in D_1_ receptor accumulation in the pathologic striatum compared with the contralateral striatum (24). On the other hand, there was a significant increase in D_2_ binding potential in the striatum contralateral to the symptoms as compared with the opposite striatum. None of the patients was on any anti-Parkinsonism medication.

Kosaka et al. performed [^11^C]NNC112 and [^11^C]SCH23390 PET imaging in six patients with schizophrenia in severe residual phase with chronic antipsychotic treatment and twelve healthy age-matched controls on the same subjects. The D_1_ binding potential (BP_ND_)values of both tracers in the frontal cortex, anterior cingulate, temporal cortex and striatum of the patients were significantly lower (21-31%) than those of the healthy controls (P < 0.001).

20361984

[^11^C]SCH 23390 PET is useful for objective monitoring of D_1_ receptor density and drug occupancy in patients with dopaminergic disorders. Internal dosimetry data for [^11^C]SCH 23390 in humans are not available in the literature.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Hyttel J., Arnt J., van den Berghe M. (1989). Selective dopamine D1 and D2 receptor antagonists. Psychopharmacol Ser.
6 Halldin C., Stone-Elander S., Farde L., Ehrin E., Fasth K.J., Langstrom B., Sedvall G. (1986). Preparation of 11C-labelled SCH 23390 for the in vivo study of dopamine D-1 receptors using positron emission tomography. Int J Rad Appl Instrum [A].
7 Hyttel J. (1983). SCH 23390 - the first selective dopamine D-1 antagonist. Eur J Pharmacol.
8 Billard W., Ruperto V., Crosby G., Iorio L.C., Barnett A. (1984). Characterization of the binding of 3H-SCH 23390, a selective D-1 receptor antagonist ligand, in rat striatum. Life Sci.
9 Hall H., Farde L., Sedvall G. (1988). Human dopamine receptor subtypes--in vitro binding analysis using 3H-SCH 23390 and 3H-raclopride. J Neural Transm.
10 Hyttel J. (1989). Parallel decrease in the density of dopamine D1 and D2 receptors in corpus striatum of rats from 3 to 25 months of age. Pharmacol Toxicol.
11 Hess E.J., Bracha H.S., Kleinman J.E., Creese I. (1987). Dopamine receptor subtype imbalance in schizophrenia. Life Sci.
12 Suzuki M., Hatano K., Sakiyama Y., Kawasumi Y., Kato T., Ito K. (2001). Age-related changes of dopamine D1-like and D2-like receptor binding in the F344/N rat striatum revealed by positron emission tomography and in vitro receptor autoradiography. Synapse.
13 Rosa-Neto P., Doudet D.J., Cumming P. (2004). Gradients of dopamine D1- and D2/3-binding sites in the basal ganglia of pig and monkey measured by PET. Neuroimage.
14 Chan G.L., Holden J.E., Stoessl A.J., Doudet D.J., Wang Y., Dobko T., Morrison K.S., Huser J.M., English C., Legg B., Schulzer M., Calne D.B., Ruth T.J. (1998). Reproducibility of the distribution of carbon-11-SCH 23390, a dopamine D1 receptor tracer, in normal subjects. J Nucl Med.
15 Hirvonen J., Nagren K., Kajander J., Hietala J. (2001). Measurement of cortical dopamine d1 receptor binding with 11C[SCH23390]: a test-retest analysis. J Cereb Blood Flow Metab.
16 Sossi V., Holden J.E., Chan G., Krzywinski M., Stoessl A.J., Ruth T.J. (2000). Analysis of four dopaminergic tracers kinetics using two different tissue input function methods. J Cereb Blood Flow Metab.
17 Farde L., Halldin C., Stone-Elander S., Sedvall G. (1987). PET analysis of human dopamine receptor subtypes using 11C-SCH 23390 and 11C-raclopride. Psychopharmacology (Berl).
18 Farde L., Hall H. (1992). Positron emission tomography--examination of chemical transmission in the living human brain. Development of radioligands. Arzneimittelforschung.
19 Suhara T., Fukuda H., Inoue O., Itoh T., Suzuki K., Yamasaki T., Tateno Y. (1991). Age-related changes in human D1 dopamine receptors measured by positron emission tomography. Psychopharmacology (Berl).
20 Wang Y., Chan G.L., Holden J.E., Dobko T., Mak E., Schulzer M., Huser J.M., Snow B.J., Ruth T.J., Calne D.B., Stoessl A.J. (1998). Age-dependent decline of dopamine D1 receptors in human brain: a PET study. Synapse.
21 Sedvall G., Karlsson P., Lundin A., Anvret M., Suhara T., Halldin C., Farde L. (1994). Dopamine D1 receptor number--a sensitive PET marker for early brain degeneration in Huntington's disease. Eur Arch Psychiatry Clin Neurosci.
22 Andrews T.C., Weeks R.A., Turjanski N., Gunn R.N., Watkins L.H., Sahakian B., Hodges J.R., Rosser A.E., Wood N.W., Brooks D.J. (1999). Huntington's disease progression. PET and clinical observations. Brain.
23 Ginovart N., Lundin A., Farde L., Halldin C., Backman L., Swahn C.G., Pauli S., Sedvall G. (1997). PET study of the pre- and post-synaptic dopaminergic markers for the neurodegenerative process in Huntington's disease. Brain.
24 Rinne J.O., Laihinen A., Nagren K., Bergman J., Solin O., Haaparanta M., Ruotsalainen U., Rinne U.K. (1990). PET demonstrates different behaviour of striatal dopamine D-1 and D-2 receptors in early Parkinson's disease. J Neurosci Res.